# Iron oxide nanoparticles-poly-L-lysine complex

Chemical name: | Iron oxide nanoparticles-poly-L-lysine complex
Abbreviated name: | SPIO-PLL
Synonym: | Ferumoxides-PLL, Feridex-PLL, FE-PLL
Agent category: | Nanoparticle
Target: | Other
Target category: | Other
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxides
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=iron oxides + PLL)]

Transplantation of stem cells (SCs) and other mammalian cells into tissues provokes great clinical research interest in developing cell- and gene-therapeutic agents (1). In particular, SCs have unlimited self-renewal capacity, high multilineage differentiation potential, and injury site homing capability (2). Marrow-derived mesenchymal stem cells (MSCs) are multipotent SCs that can differentiate into osteocytes, chondrocytes, tenocytes, and adipocytes (2). MSCs have been widely used in regeneration of connective tissues such as bone, cartilage, and fat. Neural stem cells (NSCs) are another type of multipotent SCs that are generally propagated into floating cell clusters called neurospheres (NSs) and further differentiate into neurons, astrocytes, and oligodendrocytes (3). Embryo-derived stem cells (ESCs) are pluripotent SCs that can differentiate into virtually all cells of the human body. ESCs provide a replacement cell source to treat various diseases including age-related functional defects, hematopoietic and immune system disorders, heart failure, chronic liver injuries, diabetes, Parkinson’s and Alzheimer’s diseases, arthritis, and muscular, skin, lung, eye, and digestive disorders as well as aggressive and recurrent cancers (4). Tracking the migration of transplanted SCs in vivo becomes a critical methodology in evaluating the efficacy of SC therapy (5). Among a variety of non-invasive imaging modalities, magnetic resonance imaging (MRI) can monitor the migration of SCs as long as a few months after the transplantation of paramagnetically labeled SCs (6). With its inherent high spatial resolution, MRI provides insight into several cellular processes including localization and migration of the cells, cell survival and proliferation kinetics, and cell differentiation of de-differentiation patterns, which can aid clinical implementation of cell therapy (7).

Most paramagnetic labeling of SCs is carried out with dextran-coated super paramagnetic iron oxide nanoparticles (SPIO) because of their good biodegradability and tolerance (8). Although SPIOs are known to accumulate in Kupffer cells and reticuloendothelial cells in the spleen after intravenous administration, they cannot be used to efficiently label nonphagocytic or non-rapidly dividing mammalian cells in vitro (9). SPIOs are internalized through formation of a complex with DNA transfection agents such as poly-L-lysine (PLL) to achieve ~100% efficiency of labeling cells (8). PLL contains positive charges and forms stable complexes with the negatively charged SPIO by simply mixing SPIO with PLL in cell culture media. The formation of the SPIO-PLL complex via electrostatic interaction alters the electrostatic interactions between the SPIO and the cell membrane, which initiates endocytosis and/or macropinocytosis of SPIO-PLL complexes (1). PLL (molecular weight ~400 kDa) is available from many manufacturers (8). Ferumoxides (SPIOs) as MRI contrast agents approved by the U.S. Food and Drug Administration for detection of liver lesion are also commercially available, including Feridex and Endorem (8). For having a dextran-coating, these commercial SPIOs can be directly used in the process of cell labeling. This labeling method can upload 10–20 pg Fe to each cell and appears not to affect the cell viability or the proliferation capacity (9). SPIO is usually detected as signal-loss (hypointense) areas in T_2_*-weighted images in MRI. The substantial magnetic susceptibility effect of SPIO leads to a hypointense area much larger than the actual size of the particles, known as a “blooming effect” (10). This effect permits detection of ~20 labeled cells per 1,000 cells in a voxel (1 mm slice thickness, ~300 μm in plane resolution) by MRI at 1.5 T (9), the proliferation of labeled cells at up to 18 weeks (6), and a single labeled cell in mice at ultra-high magnetic fields (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Iron oxides + PLL)+AND+synthesis%0D%0A)]

The SPIO-PLL complex is made by simply mixing SPIO and PLL in solution (8). Depending on the cell types, the ratio of SPIO to PLL varies between 1:0.03 and 1:0.06. Frank’s group described a detailed procedure of labeling various SCs with commercial Feridex (SPIO) and a 388-kDa PLL as the starting materials (8, 9). For adherent cells such as human cervical carcinoma (HeLa) cells, human MSCs, and rhesus ESCs, or for rapidly growing cells such as small-cell lung carcinoma cells and human marrow-derived neural competent cells, the optimal concentration was 25 μg Fe/ml Feridex and 0.75 μg/ml PLL. For mononuclear cells such as mouse and marmoset T lymphocytes, hematopoietic SCs (CD34+), and mouse Sca1+, the optimal concentration was 25 μg Fe/ml Feridex and 1.5 μg/ml PLL. The labeling efficiency was ~100% for both incubation conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Iron oxides + PLL)+AND+%22in+vitro%22)]

The iron content in various labeled cells was quantified with nuclear magnetic resonance T_2_ relaxometry (9). Typically, intracytoplasmic endosomal iron was found to be 1–3 pg/cell in T cells, 4–10 pg/cell in HeLa cells, and 15–20 pg/cell in MSCs, compared to 0.01–0.1 pg/cell in unlabeled cells (endogenous iron) (9). The degradation of SPIO-PLL complexes was examined under various physiological conditions (12). After mixing 25 μg Fe/ml SPIO with 0.75 μg /ml PLL in buffers of different pH levels, the T_2_ and Fe(III) concentration were measured at 0, 6, 24, 48, 72, and 96 h as well as at 7, 14, and 21 days. SPIO-PLL complexes appeared to dissolve rapidly in buffers containing sodium citrate at pH 4.5; they were less soluble in the same buffer at pH 5.5, but they were not readily soluble in buffers containing sodium acetate or in cell culture media RPMI-1640 regardless of pH. To assess the stability of SPIO-PLL complexes inside the endosomes/lysomes (12), MSCs labeled with SPIO-PLL were analyzed by electron microscopy, T_2_ relaxometry at 1.0 T, and MRI at 1.5 T. MSCs were incubated overnight in RPMI-1640 media containing 25 μg/ml SPIO and 0.75 μg/ml PLL. The labeled cells were collected at different time points from 1 h to 5 days for analysis. Electron microscopic imaging showed degraded SPIO-PLL in some intracellular endosomes/lysosmes between days 3 and 5. Some endosomes containing SPIO-PLL were found to fuse with lysosomes to cause rapid dissociation of SPIO within lysosomes at low pH. The viability of labeled HeLa/MSC was examined at days 1, 3, 7, and 15, and its value was ~100% at day 15. The paramagnetic labeling appeared not to alter the differentiation capacity of MSCs compared with the unlabeled cells.

The SPIO-PLL human central nervous system stem cell–derived NSs (hCNS-NSs) were tested for labeling efficiency, cell proliferation, cell differentiation, and electrophysiological behavior (6). The labeling efficiency was determined with Prussian blue staining, one of the most sensitive histochemical tests for iron-positive cells, which indicated that ~98% of cells were labeled. The cell viability was 92 ± 3% for SPIO-labeled hCNS-NSs compared with 96 ± 2% for unlabeled hCNS-NSs. No difference in the proliferation rate was observed between SPIO-labeled and unlabeled hCNS-NSs. The SPIO content per cell was approximately halved every 3 days in culture, which was consistent with cell-doubling time. After 10-day differentiation, an average of 35.5 ± 4% of the cells were Nestin-positive, 56.2 ± 7.7% were β-tubulin-positive, and 19.4 ± 3.5% were glial fibrillary acidic protein–positive in the labeled cells. There was no statistically significant difference between the labeled and unlabeled cells. These percentages were found to be similar to the unlabeled cells. After 28-day differentiation, whole-cell patch-clamp recording showed no difference in electrophysiological characteristics for the labeled and unlabeled cells. Cell differentiation was also examined in SPIO-PLL–labeled MSCs (13), which exhibited an unaltered viability, proliferation similarity, normal adipogenic and osteogenic differentiation, but a marked inhibition of chondrogensis. The blocking of chondrogenic activity appeared to be mediated by the SPIO, not by the transfection agent PLL. MSCs of canine, porcine, or human (hMSC) origins demonstrated similar labeling efficiency (13), indicating the non-specific nature of SPIO uptake among different species. The long-term viability, growth rate, and apoptotic indexes of the labeled MSCs appeared to be unaffected by the endosomal incorporation of SPIO compared with the unlabeled cells. In non-dividing hMSCs, endosomal SPIO could be detected after 7 weeks; however, in rapidly dividing cells, intracellular iron disappeared at five to eight divisions (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Iron oxides + PLL) +AND+rodentia)]

Yocum et al. studied the effect of SPIO-PLL–labeled MSCs on the physiology of rats after intravenous injection (15). hMSCs were incubated with 25 μg Fe/ml SPIO and 0.75 μg/ml PLL (molecular weight = 388 kDa). After the rats (n = 25, 125–250 g) received 2 × 10^6^ labeled hMSCs (~10 pg Fe per cell) in 0.5 ml of phosphate-buffered saline, a series of measurements were conducted for 42 days, including complete blood counts, liver and renal function tests, and serum electrolyte and iron concentration measurements. The administration of labeled hMSCs appeared not to have a significant effect on hematology, blood chemistry indicators, or organ function. Hemoglobin concentration and mean corpuscular volume were altered significantly. Other properties such as serum electrolyte and iron concentrations changed significantly. To determine the half-life of labeled hMSCs in the circulation, 100 μl of venous blood was collected from the inferior vena cava before injection of the labeled hMSCs and at 1, 5, 15, 30, 60, and 120 min after injection of the labeled hMSCs. Prussian blue–positive MSCs were not detected at 15 min after injection, which was attributed to the homing of hMSCs to the liver, spleen, bone marrow, and other organs.

Ben-Hur et al. conducted a biodynamic study of the migration of transplanted cells to injured sites in chronic experimental autoimmune encephalomyelitis (EAE) mice (n=8) (16). Syngeneic mouse NSs (SM-NSs) or human ESC-derived NSs (hESC-NSs) were incubated with 25 μg Fe/ml Feridex and 0.375 μg/ml PLL (molecular weight = 388 kDa) and differentiated in vitro for 5 days. The lineage fate was immunostained with a lineage-specific marker to verify that the paramagnetic labeling did not affect multipotency of the cells. Transplantation of the labeled cells was carried out on day 6 after EAE induction. Using a stereotaxic device, 150 SM-NSs (~100 cells per sphere) in 5 μl were transplanted into the lateral ventricle of eight EAE mice, and 250 hESC-NSs (~3,000 cells/sphere) were transplanted into both lateral ventricles of another eight EAE mice. MRI was performed at 4.7 T on days 1–2, 6–7, 13–14, and 30 after the transplantation to assess the different stages of disease. The results demonstrated that the labeled cell migration occurred along with white matter tracts (especially the corpus callosum, fimbria, and internal capsule), predominantly early in the acute phase of disease in an asymmetric manner. The distance of cell migration correlated well with clinical severity of disease and the number of microglia in the white matter tracts.

Guzman et al. examined the migration patterns of SPIO-labeled hCNS-NSs after they were transplanted into the brains of newborn and adult (injured and uninjured) rodents (mice and rats) by MRI at 4.7 T (6). Compared with the unlabeled cells, the SPIO-labeled hCNS-NSs appeared to have similar extent of survival, migration, integration, and differentiation after transplantation. All measurements of viability were performed in vitro. The test to check if the cells were alive was conducted through the test of differentiation then followed by histological analysis. In neonatal NOD-SCID mice (n = 16), the migration of SPIO-labeled hCNS-NSs spread along the natural tracts and differentiated into neurons and glia. hCNS-NSs were detected with MRI in the ventricular system immediately after transplantation. The labeled hCNS-NSs were found to distribute into the lateral and the fourth ventricle 3 weeks later and to migrate from the subventricular zone to the corpus callosum and olfactory glomerulus 9 and 12 weeks later. The migration remained visible at up to 18 weeks, which was further confirmed by double immunofluorescence stainings using human-specific and neuronal-specific antibodies. In stroke-injured rat brains (n = 10), transplanted SPIO-labeled hCNS-NSs were detected on T_2_*-weight images at up to 5 weeks. To validate the MRI signal of labeled cells, dead and viable labeled cells were implanted on the left and right striatum of immunosuppressed rats, respectively. MRI was performed from day 2 to day 35. The day 2 images exhibited bilateral hypointense areas, which represented the grafts. Whereas minimal signal changes over 35 days were observed on the side with viable cells, a marked reduction in signal strength and graft volume appeared on the side with dead cells. For the nanoparticles in the dead cells, they could be endocytosized by macrophages, generating less intense contrast change than groups of viable cells containing many packed nanoparticles (11).

Amsalem et al. tracked the migration of SPIO-PLL–labeled MSCs in rats (n = 29) with myocardial infarction on a 0.5 T imager (17). Rat MSCs (rMSCs) were isolated from bone marrow of rats and labeled with SPIO-PLL. Seven days after the induction of myocardial infarction, 2 × 10^6^ SPIO-labeled MSCs were injected into the anterior wall of the left ventricle. MRI was performed at 1, 2, and 4 weeks after cell delivery. Hypointensities induced by labeled rMSCs were visible at up to 4 weeks. Ju et al. conducted intrasplenic transplantation of 6 × 10^6^ labeled MSCs cells into rats (n = 6) with liver damage (18). MRI was performed at 1.5 T to track the migration of the cells. The contrast/noise ratio on T_2_*-weighted images of the liver appeared to decrease significantly 3 h after injection of the labeled MSCs; this ratio returned gradually to the level achieved without labeled cell injection in 14 days. Ko et al. reported a migration study of scaffold model in mice (n = 30) at 1.5 T (10). Gelatin sponge that contained SPIO-PLL–labeled hMSCs was implanted in nude mice (6-week-old BALB/C-nude mice). The hypointense areas were observable at up to 4 weeks on T_2_*-weighted images.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Kraitchman et al. used MRI at 1.5 T to track the migration of labeled MSCs in swine (sMSCs) with myocardial infarction (19). sMSCs were incubated with 25 μg Fe/ml Feridex and 375 ng/ml PLL (molecular weight = 275 kDa) for 2 h. The labeled sMSCs were injected intramyocardially into swine (n = 5, 25–35 kg), guided by x-ray fluoroscopy. The injected animal had a volume of 4–16 ml at a concentration of 7 × 10^6^ to 1 × 10^7^ cell/ml. The total number of cells injected ranged from 2.8 × 10^7^ to 1.6 × 10^8^. At 24 h after injection, images of the heart exhibited ovoid hypointense lesions with sharp borders at the injection sites. One week later, the delineation of the borders became less clear. The hypointense lesions were expanded by 15% with a 24% deduction in contrast.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Iron oxides + PLL) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Iron oxides + PLL) +AND+human)]

No publication is currently available.

### NIH Support

NS 045062, HL 63439, HL 04193, HL 45090, HL 65455, NS 27292, NS37520

## References

1 Politi L.S., Bacigaluppi M., Brambilla E., Cadioli M., Falini A., Comi G., Scotti G., Martino G., Pluchino S. (2007). Magnetic-resonance-based tracking and quantification of intravenously injected neural stem cell accumulation in the brains of mice with experimental multiple sclerosis. Stem Cells.
2 Deans R.J., Moseley A.B. (2000). Mesenchymal stem cells: biology and potential clinical uses. Exp Hematol.
3 Shanthly N., Aruva M.R., Zhang K., Mathew B., Thakur M.L. (2006). Stem cells: a regenerative pharmaceutical. Q J Nucl Med Mol Imaging.
4 Mimeault M., Hauke R., Batra S.K. (2007). Stem cells: a revolution in therapeutics-recent advances in stem cell biology and their therapeutic applications in regenerative medicine and cancer therapies. Clin Pharmacol Ther.
5 Dousset V., Tourdias T., Brochet B., Boiziau C., Petry K.G. (2008). How to trace stem cells for MRI evaluation?. J Neurol Sci.
6 Guzman R., Uchida N., Bliss T.M., He D., Christopherson K.K., Stellwagen D., Capela A., Greve J., Malenka R.C., Moseley M.E., Palmer T.D., Steinberg G.K. (2007). Long-term monitoring of transplanted human neural stem cells in developmental and pathological contexts with MRI. Proc Natl Acad Sci U S A.
7 Swijnenburg R.-J., van der Bogt K.E., Sheikh A.Y., Cao F. (2007). , and W.J. C., Clinical hurdles for the transplantation of cardiomyocytes derived from human embryomic stem cells: role of molecular imaging.
8 Bulte J.W., Arbab A.S., Douglas T., Frank J.A. (2004). Preparation of magnetically labeled cells for cell tracking by magnetic resonance imaging. Methods Enzymol.
9 Arbab A.S., Bashaw L.A., Miller B.R., Jordan E.K., Bulte J.W., Frank J.A. (2003). Intracytoplasmic tagging of cells with ferumoxides and transfection agent for cellular magnetic resonance imaging after cell transplantation: methods and techniques. Transplantation.
10 Ko I.K., Song H.T., Cho E.J., Lee E.S., Huh Y.M., Suh J.S. (2007). In vivo MR imaging of tissue-engineered human mesenchymal stem cells transplanted to mouse: a preliminary study. Ann Biomed Eng.
11 Shapiro E.M., Sharer K., Skrtic S., Koretsky A.P. (2006). In vivo detection of single cells by MRI. Magn Reson Med.
12 Arbab A.S., Wilson L.B., Ashari P., Jordan E.K., Lewis B.K., Frank J.A. (2005). A model of lysosomal metabolism of dextran coated superparamagnetic iron oxide (SPIO) nanoparticles: implications for cellular magnetic resonance imaging. NMR Biomed.
13 Kostura L., Kraitchman D.L., Mackay A.M., Pittenger M.F., Bulte J.W. (2004). Feridex labeling of mesenchymal stem cells inhibits chondrogenesis but not adipogenesis or osteogenesis. NMR Biomed.
14 Arbab A.S., Bashaw L.A., Miller B.R., Jordan E.K., Lewis B.K., Kalish H., Frank J.A. (2003). Characterization of biophysical and metabolic properties of cells labeled with superparamagnetic iron oxide nanoparticles and transfection agent for cellular MR imaging. Radiology.
15 Yocum G.T., Wilson L.B., Ashari P., Jordan E.K., Frank J.A., Arbab A.S. (2005). Effect of human stem cells labeled with ferumoxides-poly-L-lysine on hematologic and biochemical measurements in rats. Radiology.
16 Ben-Hur T., van Heeswijk R.B., Einstein O., Aharonowiz M., Xue R., Frost E.E., Mori S., Reubinoff B.E., Bulte J.W. (2007). Serial in vivo MR tracking of magnetically labeled neural spheres transplanted in chronic EAE mice. Magn Reson Med.
17 Amsalem Y. Mardor Y. Feinberg M.S. Landa N. Miller L. Daniels D. Ocherashvilli A. Holbova R. Yosef O. Barbash I.M. Leor J. Iron-oxide labeling and outcome of transplanted mesenchymal stem cells in the infarcted myocardium Circulation 2007 116Suppl11 I38 45 17846324
18 Ju S., Teng G.J., Lu H., Zhang Y., Zhang A., Chen F., Ni Y. (2007). In vivo MR tracking of mesenchymal stem cells in rat liver after intrasplenic transplantation. Radiology.
19 Kraitchman D.L., Heldman A.W., Atalar E., Amado L.C., Martin B.J., Pittenger M.F., Hare J.M., Bulte J.W. (2003). In vivo magnetic resonance imaging of mesenchymal stem cells in myocardial infarction. Circulation.